# Gd-DTPA-Bz-poly(α,L-glutamic acid)

Chemical name: | Gd-DTPA-Bz-poly(α, L-glutamic acid)
Abbreviated name: | GdLPG
Synonym: | L-PG-DTPA-Gd, PG-Bz-DTPA-Gd
Agent category: | Polymer
Target: | Other
Target category: | Other – blood pool agent
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal/contrast: | Gadolinium
Activation: | No
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=L-PG-DTPA-Gd)]

Blood pool contrast agents (BPCAs) used in magnetic resonance imaging (MRI) are paramagnetic contrast agents designed to remain in the blood for a prolonged time (1). Macromolecule-based gadolinium (Gd(III)) complexes are excellent candidates for BPCAs in the context of overcoming the limitations of low molecular weight contrast agents, such as the rapid elimination for blood pool, nonspecific extravasation into surrounding tissue, and poor relaxation enhancement efficiency (2). BPCAs can significantly increase the T_1_ relaxation rate because of their elongation of rotation correlation time (τ_R_) (3), and they can produce persistently enhanced signals in a long acquisition time. In addition to the applications in magnetic resonance angiography, BPCAs are used to target necrotic myocardium (4, 5), to access myocardial viability (6), and to detect various tumors (7, 8). The size of BPCAs controls their extravasation from the leaky vasculatures into the surrounding interstitia via the enhanced permeability and retention (EPR) effect (9). This often occurs wherever an inflammatory response is present, such as cancer, arthritis, and vascular diseases (2). On the other hand, the degradation and clearance of BPCAs from the body creates a safety issue; i.e., the tissue retention-induced toxicity of BPCAs is a primarily critical factor for the use of BPCAs in clinics. Thus, the development of biodegradable BPCAs becomes very important (10).

Poly(α,L-glutamic acid) (PG) is an anionic biocompatible macromolecule that has been used for drug delivery in a variety of clinical trials (11). In PG, the naturally occurring L-glutamic acids are linked by amide bonds, which are readily degradable by lysosomal enzymes into its basic unit (L-glutamic acid) in cells. The pendant free γ-carboxyl in each repeating unit of PG provides a functional group for attachment of drugs, therapeutic agents, and/or imaging contrast agents. Gd-Labeled diethylenetriamine pentaacetic acid-Bz-PG (GdLPG) is a PG attached with numerous Gd-DTPAs, which can be used as BPCAs in MRI (12, 13).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( L-PG-DTPA-Gd)+AND+synthesis%0D%0A)]

Wen et al. described the detailed synthesis of GdLPG (13). PG (M_n_ ~42 kDa) was conjugated with p-aminobenzyldiethylenetriamine pentaacetic (acid) tert-butyl ester in the presence of 1,3-diisopropylcarbodiimde as the coupling reagent. The produced PG-BZ-DTPA, in which 50 of 278 glutamic acid units were attached to Bz-DTPA, was reacted with GdCl_3_ to produce GdLPG, which has a calculated M_w_ of 77 kDa and contains 12.3% Gd content or 0.22 mol Gd/mol COOH.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( L-PG-DTPA-Gd)+AND+%22in+vitro%22)]

The T_1_ and T_2_ relaxivities of GdLPG were measured at different magnetic fields (12, 13). The T_1_ relaxivity was 21 Gd mM^-1^s^-1^ at 1.5 T and 8.1 Gd mM^-1^s^-1^ at 4.7 T, whereas the T_2_ relaxivity was 27 Gd mM^-1^s^-1^ at 1.5 T and 21.5 Gd mM^-1^s^-1^ at 4.7 T.

The degradation of GdLPG in the presence of cathepsin B in vitro was evaluated as a function of time (13). GdLPG degraded rapidly, as shown by the complete disappearance of the main polymeric peak within 24 h.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( L-PG-DTPA-Gd) +AND++rodentia)]

Wen et al. studied the biodistribution of GdLPG in mice using ^111^In-labeled GdLPG (13). C3Hf/Kam mice (20–25 g, n = 4) bearing MCa-4 tumors ~8 mm in diameter were injected intravenously with ^111^In-labeled GdLPG (0.4 mg, 15 μCi). Animals were euthanized at 5 min, 2 h, 24 h, and 49 h after injection, and the tissues were harvested for gamma counting. Immediately after injection, GdLPG exhibited a high blood activity of 28.50 ± 1.66% injected dose per gram (% ID/g) at 5 min, which decreased to 7.72 ± 0.28% ID/g at 2 h and appeared to be negligible after 24 h. At 2–48 h the kidney exhibited the highest uptakes: 8.4 ± 0.37% ID/g at 5 min, 20.77 ± 4.70% ID/g at 2 h, 17.54 ± 2.70% ID/g at 24 h, and 10.07 ± 0.61% ID/g at 48 h. The liver exhibited moderate uptake: 5.14 ± 0.29% ID/g at 5 min, 8.3 ± 1.47% ID/g at 2 h, 11.10 ± 1.72% ID/g at 24 h, and 9.36 ± 0.43% ID/g at 48 h. The distribution in the tumor was 0.73 ± 0.14% ID/g at 5 min, 2.42 ± 0.77% ID/g at 2 h, 1.74 ± 0.54% ID/g at 24 h, and 2.27 ± 0.22% ID/g at 48 h. The distribution in the muscle was low at all time points (<1% ID/g).

Wen et al. examined the relaxation enhancement of GdLPG in vivo at 1.5 T (13). Mice bearing MCa-4 tumors were intravenously injected with GdLPG at a dose of 0.04 mmol Gd/kg. T_1_-Weighted images were collected before injection and at 10 min, 2 h, and 24 h after injection. The blood vessels such as the vena cava as well as myocardial, hepatic, lung, and renal perfusion were clearly visualized at 2 h and returned to the precontrast level at 24 h. However, the contrast in some tumoral regions appeared to be enhanced at 24 h, suggesting an enhanced permeability and retention of GdLPG in solid tumors.

Jackson et al. used GdLPG to examine solid tumors in vivo at 4.7 T (12). CD-1 nude mice bearing Colo-205 tumors were injected intravenously with GdLPG at a dose of 0.04 mmol Gd/kg on days 0, 2, 4, and 7. MRI images were collected before injection and 2–4 days after each injection. The images acquired on day 2 (2 days after the first dose), day 4 (2 days after the second dose), day 7 (3 days after the third dose), and day 11 (4 days after the fourth and last dose) all exhibited a similarly enhanced pattern in the tumoral regions. In particular, the central zone of the tumor was significantly enhanced. At the end of the final imaging session, the mice were euthanized and the tumors were excised immediately for histological analysis. A hematoxylin and eosin– (H&E) stained section of the tumor, which was in the same plane as the MRI, showed that the areas of necrosis closely resembled the areas with enhanced MRI signals. This result suggested a significant accumulation of GdLPG in necrotic tissues.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( L-PG-DTPA-Gd) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( L-PG-DTPA-Gd) +AND+human)]

No publication is currently available.

### NIH Support

CA90810, CA 16672, EB00174

## References

1 Weinmann H.J., Ebert W., Misselwitz B., Schmitt-Willich H. (2003). Tissue-specific MR contrast agents. Eur J Radiol.
2 Mohs A.M., Lu Z.R. (2007). Gadolinium(III)-based blood-pool contrast agents for magnetic resonance imaging: status and clinical potential. Expert Opin Drug Deliv.
3 Lauffer R.B. (1987). Paramagnetic metal complexes as water proton relaxation agents for NMR imaging:Theory and design. Chem. Rev.
4 Kroft L.J., de Roos A. (1999). Blood pool contrast agents for cardiovascular MR imaging. J Magn Reson Imaging.
5 Muhler A. (1995). Assessment of myocardial perfusion using contrast-enhanced MR imaging: current status and future developments. Magma.
6 Schmiedl U., Moseley M.E., Sievers R., Ogan M.D., Chew W.M., Engeseth H., Finkbeiner W.E., Lipton M.J., Brasch R.C. (1987). Magnetic resonance imaging of myocardial infarction using albumin-(Gd-DTPA), a macromolecular blood-volume contrast agent in a rat model. Invest Radiol.
7 Kiessling F., Morgenstern B., Zhang C. (2007). Contrast agents and applications to assess tumor angiogenesis in vivo by magnetic resonance imaging. Curr Med Chem.
8 Daldrup H.E., Roberts T.P., Muhler A., Gossmann A., Roberts H.C., Wendland M., Rosenau W., Brasch R.C. (1997). , and , .
9 Weissleder R., Bogdanov A., Tung C.H., Weinmann H.J. (2001). Size optimization of synthetic graft copolymers for in vivo angiogenesis imaging. Bioconjug Chem.
10 Lu Z.R., Wang X., Parker D.L., Goodrich K.C., Buswell H.R. (2003). Poly(l-glutamic acid) Gd(III)-DOTA conjugate with a degradable spacer for magnetic resonance imaging. Bioconjug Chem.
11 Li C. (2002). Poly(L-glutamic acid)--anticancer drug conjugates. Adv Drug Deliv Rev.
12 Jackson E.F., Esparza-Coss E., Wen X., Ng C.S., Daniel S.L., Price R.E., Rivera B., Charnsangavej C., Gelovani J.G., Li C. (2007). Magnetic resonance imaging of therapy-induced necrosis using gadolinium-chelated polyglutamic acids. Int J Radiat Oncol Biol Phys.
13 Wen X., Jackson E.F., Price R.E., Kim E.E., Wu Q., Wallace S., Charnsangavej C., Gelovani J.G., Li C. (2004). Synthesis and characterization of poly(L-glutamic acid) gadolinium chelate: a new biodegradable MRI contrast agent. Bioconjug Chem.